# ^99m^Tc-Hydrazinonicotinamide-galactosyl-chitosan

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-galactosyl-chitosan
Abbreviated name: | ^99m^Tc-HGC
Synonym:
Agent category: | Compound
Target: | Asialoglycoprotein receptors (ASGP-Rs)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4502251), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/186910312) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=432) for more information about ASGP-R.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC)]

Asialoglycoprotein (ASGP) is specifically taken into mammalian hepatocytes by binding to ASGP receptors (ASGP-Rs) (1). The galactosyl moiety of ASGP is recognized on the surface of hepatocytes and is bound by ASGP-R. The ASGP–ASGP-R complex on the cell surface is subsequently taken into cytoplasm by endocytosis and transferred to lysosomes. ASGP-R is then dissociated from ASGP and recycled to the cell surface. ASGP is degraded in the lysosomes and excreted into the bile. The number of ASGP-Rs on the hepatocytes of individuals with liver disease decreases and is thus considered a good indicator for the evaluation of liver function. Because ASGP-R recognizes galactose, ^99m^Tc-diethylenetriamine pentaacetic acid-galactosyl-human serum albumin (^99m^Tc-GSA) (2, 3) and ^99m^Tc-galactosyl-neoglycoalbumin (^99m^Tc-NGA) (4) are ASGP-R probes that accumulate specifically in the liver and are used for liver scintigraphy to determine liver mass and function. Chitosan is a linear polysaccharide composed of D-glucosamine and N-acetylglucosamine subunits with numerous amine groups of D-glucosamine for ligand conjugation. Kim et al. (5) conjugated hydrazinonicotinamide (HYNIC) and galactose (via lactobionic acid) to deacetylate chitosan for radiolabeling with ^99m^Tc to form ^99m^Tc-HYNIC-galactosyl-chitosan (^99m^Tc-HGC) for imaging ASGP-R expression in the liver.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+synthesis)]

Deacetylated chitosan (5 kDa) was incubated with lactobionic acid, 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide hydrochloride, and N-hydroxysuccinimide for 48 h at room temperature (5). The resulting galactosylated chitosan (GC) was purified with dialysis and incubated with 3 M excess succinimidyl HYNIC in 0.2 M borate buffer (pH 8.2) for 5 h at room temperature. HYNIC-GC (HGC) was isolated with dialysis. HGC (200 µg) was incubated with 74 MBq (2 mCi) ^99m^Tc-sodium pertechnetate, tricine, and stannous chloride for 30 min at room temperature. ^99m^Tc-HGC conjugates were isolated with column chromatography with >94% labeling efficiency. ^99m^Tc-HGC conjugates were stable in saline up to 6 h. The amount of galactose in GC was 7 mol% and in HGC was 3 mol%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+in+vitro)]

No publication is currently available

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+rodentia)]

Kim et al. (5) performed ex vivo biodistribution studies in normal mice (n = 3/group) after intravenous injection of ^99m^Tc-HGC at 10, 60, and 120 min. The initial tracer accumulation in the liver was 13.2% injected dose per gram (ID/g) at 10 min, 16.1% ID/g at 60 min, and 16.6% ID/g at 120 min after injection. The kidneys had the highest accumulation with 32.2%, 25.6%, and 23.3% ID/g at these time points, respectively. ^99m^Tc-HGC was largely cleared by the kidneys. The stomach, intestine, heart, lung, muscle, blood, and spleen all showed relatively low accumulation. Single-photon emission computed tomography scintigraphic imaging was performed in mice after intravenous injection of 2.8 MBq (0.075 mCi) ^99m^Tc-HGC at 10, 30, 60, and 120 min after injection. High accumulation was observed in the liver and kidneys within a few minutes after injection. The urinary bladder was also highly visualized. Co-injection of 0.05 mmol galactose with ^99m^Tc-HGC greatly reduced the hepatic radioactivity with minimal effect in the kidneys. Injection of ^99m^Tc-HYNIC-chitosan (non-galactosylated) showed high accumulation in the kidneys and urinary bladder with low radioactivity in the liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+human)]

No publication is currently available.

## References

1 Stockert R.J. (1995). The asialoglycoprotein receptor: relationships between structure, function, and expression. Physiol Rev.
2 Kwon A.H., Ha-Kawa S.K., Uetsuji S., Kamiyama Y., Tanaka Y. (1995). Use of technetium 99m diethylenetriamine-pentaacetic acid-galactosyl-human serum albumin liver scintigraphy in the evaluation of preoperative and postoperative hepatic functional reserve for hepatectomy. Surgery.
3 Wu J., Ishikawa N., Takeda T., Tanaka Y., Pan X.Q., Sato M., Todoroki T., Hatakeyama R., Itai Y. (1995). The functional hepatic volume assessed by 99mTc-GSA hepatic scintigraphy. Ann Nucl Med.
4 Vera D.R., Stadalnik R.C., Krohn K.A. (1985). Technetium-99m galactosyl-neoglycoalbumin: preparation and preclinical studies. J Nucl Med.
5 Kim E.M., Jeong H.J., Kim S.L., Sohn M.H., Nah J.W., Bom H.S., Park I.K., Cho C.S. (2006). Asialoglycoprotein-receptor-targeted hepatocyte imaging using 99mTc galactosylated chitosan. Nucl Med Biol.